# ^68^Ga-CHX-A”-Rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_

Chemical name: | ^68^Ga-CHX-A”-Rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_
Abbreviated name: | ^68^Ga-CHX-A”-ReCCMSH(Arg^11^)
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 (MC-1) receptor (MC1R)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the Melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH)]

Malignant melanoma is the most deadly form of skin cancer (1). Early and accurate diagnosis is necessary for surgery and successful treatment (2). The melanocortin (MC) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (3). Most cutaneous cell types express MC receptors, pro-opiomelanocortin (POMC), and prohormone convertases, and they also release MCs. Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily, and these receptors have been found to be overexpressed in melanoma cells (4, 5). α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and the pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (6) in the regulation of skin pigmentation via MC1R.

Positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) in cancer has been approved by United States Food and Drug Administration with many on-going clinical trials. Although [^18^F]FDG is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (7, 8). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R that is overexpressed on human and mouse melanoma cells (4, 5, 7, 9, 10). N-(2-Aminoethyl)-trans-1,2-diaminocyclohexane-N,N”,N”’-pentaacetic acid (CHX-A”) has been successfully coupled to α-MSH peptide analogs for radiolabeling with a variety of radionuclides (7, 11, 12). A rhenium-cyclized α-MSH analog, Re-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_ (ReCCMSH(Arg^11^)), was conjugated with CHX-A” (CHX-A”-ReCCMSH(Arg^11^)) and radiolabeled with ^68^Ga (^68^Ga-CHX-A”-ReCCMSH(Arg^11^)) as a potential molecular imaging agent to target melanoma (13).Rhenium-mediated cyclization exhibits significantly reduced nonspecific renal radioactivity accumulation high tumor uptake and retention coupled with rapid clearance kinetics, compared with its free sulfhydryl and disulfide bond–containing counterparts (10). ^68^Ga is a positron emitter with a physical half-life of 68 min and is suitable for PET imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+and+synthesis)]

Wei et al. (13) reported the synthesis of ^68^Ga-CHX-A”-ReCCMSH(Arg^11^). The CCMSH(Arg^11^) peptide was synthesized using standard Fmoc chemistry on an amide resin with a peptide synthesizer. CCMSH(Arg^11^) was then reacted with 2 M excess of the glutaric acid succinimidyl ester derivative of CHX-A” to the N-terminus of CCMSH(Arg^11^) to form CHX-A”-CCMSH(Arg^11^). A mixture of CHX-A”-CCMSH(Arg^11^) and ReOCl_3_ (1:1.5 molar ratio) was incubated for 30 min at 85°C. The cyclized peptide, CHX-A”-ReCCMSH(Arg^11^), was purified with high-performance liquid chromatography (HPLC). For ^68^Ga labeling, a solution of 74 MBq (2 mCi) ^68^GaCl_3_ and 20 nmol CHX-A”-ReCCMSH(Arg^11^) was heated for 20 min at 85°C. Radiochemical efficiency was reported to be >95% with a specific activity of 4.33 GBq/µmol (117 mCi/µmol) at the end of purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+in+vitro)]

Chen et al. (10) determined the 50% inhibition concentration (IC_50_) value of DOTA-ReCCMSH(Arg^11^) to be 1.2 ± 0.3 nM using B16/F1 murine melanoma cells with ^125^I-(Tyr^2^)-[Nle^4^, D-Phe]α-MSH (^125^I-NDP).In comparison, the IC_50_ value of ReCCMSH(Arg^11^) was 2.9 ± 0.3 nM. Wei et al. (13) found that the IC_50_ value for CHX-A”-ReCCMSH(Arg^11^) was 3.8 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+rodentia)]

Wei et al. (13) performed biodistribution studies in female C57BL/6 mice (n = 5/group) bearing 10-day-old B16/F1 murine melanoma tumors. Each mouse received 0.37 MBq (0.01 mCi, 91 pmol) ^68^Ga-CHX-A”-ReCCMSH(Arg^11^). The tumor uptake radioactivity levels were obtained at 30 min, 1 h, and 2 h, respectively: 2.46 ± 0.41% injected dose per gram (% ID/g), 2.16 ± 0.36% ID/g, and 2.68 ± 0.69% ID/g. The tumor retention was high up to 2 h after injection. Pretreatment with 9 nmol unlabeled NDP significantly reduced the tumor uptake to 0.61 ± 0.19% ID/g (P < 0.02) at 2 h after injection. No other tissues showed significant inhibition by unlabeled NDP. The ^68^Ga-CHX-A”-ReCCMSH(Arg^11^) uptake in nontarget tissue (except the kidneys and liver) was low at 2 h. Furthermore, the radioactivity was quickly cleared from most of the tissues (except the kidneys and liver) at 2 h after injection (e.g., kidney: 10.24 ± 0.94% ID/g at 30 min and 7.39 ± 2.13% ID/g at 2 h; liver: 1.38 ± 0.30% ID/g at 30 min and 0.79 ± 0.24% ID/g at 2 h; blood: 1.72 ± 0.24% ID/g at 30 min and 0.58 ± 0.14% ID/g at 2 h; lung: 2.64 ± 0.65% ID/g at 30 min and 0.67 ± 0.10% ID/g at 2 h). The tumor/muscle and tumor/blood ratios at 2 h were 10 and 5, respectively.

PET imaging of mice bearing the B16/F1 melanoma tumors was conducted at 2 h after intravenous injection of 3.7 MBq (0.1 mCi) ^68^Ga-CHX-A”-ReCCMSH(Arg^11^). The tumor, urinary bladder, and kidneys were clearly visible. Preinjection of 9 nmol unlabeled NDP inhibited the tumor accumulation, whereas there was little inhibition of radioactivity in the kidneys. In comparison with ^86^Y-DOTA-ReCCMSH(Arg^11^), ^111^In- and ^68^Ga-CHX-A”-ReCCMSH(Arg^11^) exhibited lower liver accumulation. ^111^In- and ^86^Y-CHX-A”-ReCCMSH(Arg^11^) showed higher tumor accumulation than ^68^Ga-CHX-A”-ReCCMSH(Arg^11^), which has a lower specific activity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+human)]

No publication is currently available.

## NIH Support

Intramural Research Program, R24 CA86307, R24 CA86060, P30 CA91842

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
4 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
5 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
6 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
7 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
8 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
9 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
10 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
11 Wei L., Butcher C., Miao Y., Gallazzi F., Quinn T.P., Welch M.J., Lewis J.S. (2007). Synthesis and biologic evaluation of 64Cu-labeled rhenium-cyclized alpha-MSH peptide analog using a cross-bridged cyclam chelator. J Nucl Med.
12 Wei L., Miao Y., Gallazzi F., Quinn T.P., Welch M.J., Vavere A.L., Lewis J.S. (2007). Gallium-68-labeled DOTA-rhenium-cyclized alpha-melanocyte-stimulating hormone analog for imaging of malignant melanoma. Nucl Med Biol.
13 Wei L., Zhang X., Gallazzi F., Miao Y., Jin X., Brechbiel M.W., Xu H., Clifford T., Welch M.J., Lewis J.S., Quinn T.P. (2009). Melanoma imaging using 111In-, 86Y- and 68Ga-labeled CHX-A''-Re(Arg11)CCMSH. Nucl Med Biol.